# 3-Carbamoyl-2,2,5,5-tetramethyl-1-pyrrolidinyl-N-oxyl

Chemical name: | 3-Carbamoyl-2,2,5,5-tetramethyl-1-pyrrolidinyl-N-oxyl
Abbreviated name: | 3CP
Synonym: | 3-Carbamoyl-PROXYL, 3-carbamoyl-2,2,5,5-tetramethyl-1-pyrrolidinyl-N-oxy, 3-carbamoyl-2,2,5,5-tetramethyl-1-pyrrolidin-1-yl-N-oxy free radical
Agent category: | Small molecule
Target: | Other
Target category: | Other -reactive oxygen species (ROS)
Method of detection: | Electron paramagnetic resonance imaging (EPRI), magnetic resonance imaging (MRI), proton electron double resonance imaging (PEDRI), Overhauser-enhanced MRI (OMRI)
Source of signal/contrast: | Nitroxide radicals
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=3-Carbamoyl-PROXYL)]

Reactive oxygen species (ROS) are various free radicals generated in a biological milieu (1, 2). They are propagated through a cascade of reactions in the pathogenesis in many diseases, including cancer, stroke, atherosclerosis, ischemia-reperfusion injury, Alzheimer’s disease, diabetic vascular diseases, and inflammatory diseases (2). In particular, ROS interact with glutathione (GSH), NADPH, and ascorbates to maintain cellular redox status (3). Therefore, the distribution of ROS in tissue can be used as a surrogate marker to characterize the redox status/environment in disease-related physiological and pathological conditions (1). Because all free radicals contain unpaired electrons, the electron paramagnetic resonance (EPR) technique, also called electron spin resonance (ESR), is specific for detecting and quantifying ROS (2). EPR spectra can provide a wealth of information for unequivocal identification of free radicals, such as fine, hyperfine, and superhyperfine structures, g-factor, and lineshape (2). EPR imaging (EPRI) technique allows for non-invasive mapping of free radicals in animals/organs (4).

EPR is fundamentally similar to nuclear magnetic resonance (NMR) (5). However, the differences in the physical and chemical properties of the resonance species (unpaired electrons versus nuclear spin) lead to three major differences in acquiring the spectra/images: gyromagnetic ratio, relaxation time, and concentration (5). The gyromagnetic ratio of an electron spin is 658 times larger than that of a proton nuclear spin, resulting in a 658-fold increase in its magnetic moment and resonant frequency. For instance, with a magnet of 0.34 T, the EPR frequency of X-band is 9.5 GHz, and the NMR frequency of proton nuclei is 14.4 MHz. As a result of the presence of strong non-resonant water absorption, a high radiofrequency such as 9.5 GHz is not suitable for examining tissue samples. Thus, much lower EPR frequencies in the range of 1.2 GHz (L-band) to 300 MHz are used instead, corresponding to a penetration depth of a few cm. The increase in the magnetic moment of electron spin provides ~700 times greater intrinsic sensitivity with EPR on a molar basis than with NMR. Because the excited electron spins relax on a nanosecond time scale, which is several orders of magnitude shorter than the nuclear spin (measured in ms), pulsed EPR (Fourier transformation EPR or time-domain EPR) is only applicable to those free radicals with an extremely narrow line, whereas most ERP spectrometers use the continuous wave technique. The lack of high concentrations of naturally occurring paramagnetic species such as free radicals often requires the addition of paramagnetic species. This in turn allows for the quantification of exogenous paramagnetic species but also requires the acquisition of anatomic information with different imaging modalities such as magnetic resonance imaging (MRI). Proton electron double resonance imaging (PEDRI), also called Overhauser-enhanced magnetic resonance imaging (OMRI)) is a double resonance technique that encodes characteristic EPR spectral information on a high-resolution MRI (6). This method uses EPR irradiation to saturate paramagnetic species and leads to polarization of water protons through the dynamic nuclear polarization (DNP) effect. The polarized protons produce enhanced signal intensity in MRI. PEDRI offers good sensitivity, high spatial resolution, and signal enhancement of approximately two orders of magnitude (7).

Nitroxides are stable organic free radicals that have a single unpaired electron delocalized between the nitrogen and the oxygen (8). The steric hindrance around the nitroxide group makes these compounds very stable. They can be obtained in pure form, and they can be stored and handled in the laboratory with no more precautions than most organic substances (9). Nitroxides used as the contrast agent in EPRI can detect the redox status on the basis of their reduction to EPR-silent hydroxylamine (10), and nitroxides have been extensively used in cells, tissues, and living animals (11). Inside cells, nitroxides are reduced to hydroxylamine by cellular antioxidants such as ascorbate, thioredoxin, reductase, ubiquinol, NADPH and GSH. Nitroxides also can function as superoxide dismutase mimics and repair DNA damage caused by ultraviolet irradiation. In addition to the use as an EPRI contrast agent, nitroxides are T_1_ relaxation agents in MRI for having an unpaired electron (12). Because their reduced form, hydroxylamine, is diamagnetic, the reduction process is accompanied by a decrease in T_1_ relaxivity. This decrease reflects the alterations in the redox status and can be used to map the redox status. Although the T_1_ relaxivity of nitroxides is much lower than that of gadolinium chelates (one unpaired electron versus seven unpaired electrons), their high cellular permeability leads to a significantly greater volume distribution in tissues and compensates for their lower relaxivity (12). Various nitroxides are designed to target different cellular compartments (8). For example, a neutral nitroxide can be distributed throughout the intracellular and extracellular environments, whereas a charged nitroxide is unable to cross the plasma membrane and can be used to measure oxygen levels in extracellular compartments. 3-Carbamoyl-2,2,5,5-tetramethyl-1-pyrrolidinyl-N-oxyl (3CP) is a neutral nitroxide that is available commercially. As a piperidine nitroxide with a line width of 1.4 Gauss and low toxicity, 3CP is suitable for EPRI and Overhauser-enhanced magnetic resonance imaging in intact animals (11).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(3-Carbamoyl-PROXYL)+AND+synthesis%0D%0A)]

3CP was synthesized in several steps (13). First, acetone was condensed with ammonia in the presence of calcium chloride. The produced 4-oxo-2,2,6,6-tetramethylpiperidine (triacetoneamine) was converted to the corresponding nitroxyl radical (4-oxo-2,2,6,6-tetramethylpiperidinoxyl) by reaction with 30% hydrogen peroxide (14). The obtained nitroxyl radicals were then treated with iodine in an alkaline medium to produce 3CP (14).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( 3-Carbamoyl-PROXYL)+AND+%22in+vitro%22)]

The T_1_ relaxivity of 3CP was determined to be 0.95 ± 0.15 mM^-1^s^-1^ in the low-field limit (<5 MHz) and decreased to 0.30 ± 0.05 mM^-1^s^-1^ at 50 MHz (15). The partition coefficient of 3CP in n-octanol/water was found to be 0.68 (16). 3CP in aqueous solution exhibited sharp triplet lines in L-band EPR spectrum (6) with hyperfine coupling constant of 14-15 G (14).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(3-Carbamoyl-PROXYL) +AND+rodentia)]

Nishino et al. used EPRI to study the in vivo pharmacokinetics of 3CP in mice (n=4) and rats (n=4) at different ages (17). Mice (4, 6, 10, 17, 37, and 52 weeks old) and rats (3, 4, 5, and 10 weeks old) were injected intravenously with 3CP at a dose of 1 mmol/kg. An L-band EPR spectrometer (1.1 GHz) was used to measure the signal of radicals in the upper abdomen of the animals. The EPR signal decay of 3CP exhibited a biphasal profile with α-phase rate constant k_1_ of 0.126 ± 0.0042 min^-1^ and β-phase rate constant k_2_ of 0.066 ± 0.0012 min^-1^. In fresh mouse blood, 3CP remained stable with a half-life (t_1/2_) of 1,286 ± 176 min. Li et al. used PEDRI to examine the distribution of 3CP in mice (35 g) (11). After intravenously injecting 0.5 ml of 100 mM 3CP solution, PEDRI was performed on a 0.38-T MRI imager (856 kHz NMR resonant frequency and 567 MHz EPR resonant frequency). 3CP was found to distribute initially in the heart, lungs, major vessels, and kidneys. Image intensity peaked at ~5 min in these areas and decayed to preinjection levels at 16 min. Okajo et al. measured the pharmacokinetics of 3CP in rats (8 weeks old) (18). After intravenous injection of 3CP at a dose of 0.3 mmol/kg, pharmacokinetics were obtained with a blood circulation monitoring method using an X-band EPR spectrometer (9.4 GHz). The EPR signal decay in blood showed a biphasic profile with k_1_ of 0.601 ± 0.043 min^-1^ and k_2_ of 0.0662 ± 0.0045 min^-1^.

Hyodo et al. used MRI to study the in vivo pharmacokinetics of 3CP in tumors (12). C3H mice (6–8 weeks old, 20–30g,) were implanted with squamous cell carcinoma (SCCVII) in the right hind leg. After intravenous injection of 3CP at a dose of 1.5 mmol/kg, T_1_-weighted images were collected on a 4.7-T MRI imager. The contrast in the tumor area increased until 2.8 min after injection and decreased after 7.8 min. The decay rate in the tumor (0.107 ± 0.020 min^-1^) was approximately two times higher than that in the normal leg (0.056 ± 0.013 min^-1^). The blood and organs were collected at 2.5, 7.5, 10, 15, and 20 min after injection, and the concentration of 3CP in tissues was assessed with the use of an X-band EPR spectrometer. The levels of nitroxide plus nitroxylamine as a function of time did not demonstrate significant change in tumor or muscle during the imaging time. Matsumoto et al. compared the pharmacokinetics of 3CP in the same tumor model as measured with EPRI with that measured with MRI (6). EPR images were collected on a 300-MHz EPR imager, and T_1_-weighted MRI images were collected on a 4.7-T MRI imager. EPRI and MRI showed similar reduction rates of 3CP, which were 0.0783 ± 0.023 min^-1^ for normal leg and 0.0870 ± 0.0233 min^-1^ for tumor leg on EPRI, and 0.0669 ± 0.0108 min^-1^ for normal leg and 0.0973 ± 0.0090 min^-1^ for tumor leg on MRI. Mikuni et al. used EPRI to examine the pharmacokinetics of 3CP in gastric carcinoma in rats (4). Rats (n = 8) with gastric cancer tumors (2–8 mm in diameter) or healthy rats (n = 6) as control were injected intravenously with 1.5 ml of 300 mM 3CP solution. EPR images were collected on a 750-MHz EPR imager after injection. The level of 3CP in the tumors was too low to be detected compared with that in the normal stomach tissue (t_1/2_ = ~8.7 ± 0.6 min).

Velayutham et al. used EPRI to examine the distribution of 3CP in rat hearts (19). The hearts of rats (140–160 g) after occlusion of the left anterior descending coronary artery were perfused with cardioplegic buffer containing 1.5 mM of 3CP. EPR images of the hearts were collected with a L-band EPR spectrometer (1.2 GHz). A loss in signal intensity was found in the ischemic region, which was further confirmed with histological measurements. Hirayama et al. used EPRI with 3CP to examine various phases of murine renal ischemia-reperfusion injury in mice deficient in NF-E2–related factors (3). After intravenous injection of 30 μmol 3CP, EPR images in the upper abdominal area were collected at 4, 6.5, 9, and 11.5 min. Compared with the pre-ischemia phase and the recovered phase, the injured phase demonstrated a remarkably prolonged decay in signal intensity.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

The physiological effects of 3CP were tested in healthy pigs (6–12 month old, 30–80 kg) (20). 3CP was injected intravenously at doses of 30 mg/kg, 150 mg/kg, and 300 mg/kg with 4 days between doses. No changes in blood pressure or heart rate were noticed. No observable clinical toxicity was found.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(3-Carbamoyl-PROXYL) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(3-Carbamoyl-PROXYL) +AND+human)]

No publication is currently available.

### NIH Support

EB004900, EB00890, EB00306, EB00254, CA78886, RR12190, GM58582, NIH intramural research program

## References

1 Soule B.P., Hyodo F., Matsumoto K., Simone N.L., Cook J.A., Krishna M.C., Mitchell J.B. (2007). Therapeutic and clinical applications of nitroxide compounds. Antioxid Redox Signal.
2 Kuppusamy P., Zweier J.L. (2004). Cardiac applications of EPR imaging. NMR Biomed.
3 Hirayama A., Nagase S. (2006). Electron paramagnetic resonance imaging of oxidative stress in renal disease. Nephron Clin Pract.
4 Mikuni T., He G., Petryakov S., Fallouh M.M., Deng Y., Ishihara R., Kuppusamy P., Tatsuta M., Zweier J.L. (2004). In vivo detection of gastric cancer in rats by electron paramagnetic resonance imaging. Cancer Res.
5 Gallez B., Swartz H.M. (2004). In vivo EPR: when, how and why?. NMR Biomed.
6 Matsumoto K., Narazaki M., Ikehira H., Anzai K., Ikota N. (2007). Comparisons of EPR imaging and T1-weighted MRI for efficient imaging of nitroxyl contrast agents. J Magn Reson.
7 Hyodo F., Murugesan R., Matsumoto K., Hyodo E., Subramanian S., Mitchell J.B., Krishna M.C. (2008). Monitoring redox-sensitive paramagnetic contrast agent by EPRI, OMRI and MRI. J Magn Reson.
8 Gallez B., Baudelet C., Jordan B.F. (2004). Assessment of tumor oxygenation by electron paramagnetic resonance: principles and applications. NMR Biomed.
9 Holtzman, J.L., ed. Spin labeling in pharmacology1984, Academic Press, INC: New York. 5.
10 Kroll C., Borchert H.H. (1999). Metabolism of the stable nitroxyl radical 4-oxo-2,2,6, 6-tetramethylpiperidine-N-oxyl (TEMPONE). Eur J Pharm Sci.
11 Li H., He G., Deng Y., Kuppusamy P., Zweier J.L. (2006). In vivo proton electron double resonance imaging of the distribution and clearance of nitroxide radicals in mice. Magn Reson Med.
12 Hyodo F., Matsumoto K., Matsumoto A., Mitchell J.B., Krishna M.C. (2006). Probing the intracellular redox status of tumors with magnetic resonance imaging and redox-sensitive contrast agents. Cancer Res.
13 Sosnovsky G., Konieczny M. (1976). Preparation of triacetoneamine (4-oxo-2,2,6,6-tetramethylpiperidine), an improved method. Synthesis.
14 Zhdanov, R.I., Nitroxyl radicals and non-radical reactions of free radicals. Bioactive spin labels, ed. R.I. Zhdanov. 1992, New York: Springer-verlag. 26.
15 Bennett H.F., Brown R.D., Koenig S.H., Swartz H.M. (1987). Effects of nitroxides on the magnetic field and temperature dependence of 1/T1 of solvent water protons. Magn Reson Med.
16 Hyodo F., Yasukawa K., Yamada K., Utsumi H. (2006). Spatially resolved time-course studies of free radical reactions with an EPRI/MRI fusion technique. Magn Reson Med.
17 Nishino N., Yasui H., Sakurai H. (1999). In vivo L-band ESR and quantitative pharmacokinetic analysis of stable spin probes in rats and mice. Free Radic Res.
18 Okajo A., Matsumoto K., Mitchell J.B., Krishna M.C., Endo K. (2006). Competition of nitroxyl contrast agents as an in vivo tissue redox probe: comparison of pharmacokinetics by the bile flow monitoring (BFM) and blood circulating monitoring (BCM) methods using X-band EPR and simulation of decay profiles. Magn Reson Med.
19 Velayutham M., Li H., Kuppusamy P., Zweier J.L. (2003). Mapping ischemic risk region and necrosis in the isolated heart using EPR imaging. Magn Reson Med.
20 Hahn S.M., Sullivan F.J., DeLuca A.M., Bacher J.D., Liebmann J., Krishna M.C., Coffin D., Mitchell J.B. (1999). Hemodynamic effect of the nitroxide superoxide dismutase mimics. Free Radic Biol Med.